# [^99m^Tc-N_4_^0-1^-bzlg^0^,D-Phe^6^,Leu-NHEt^13^,des-Met^14^]Bombesin(6–14)

Chemical name: | [^99m^Tc-N_4_^0-1^-bzlg^0^,D-Phe^6^,Leu-NHEt^13^,des-Met^14^]Bombesin(6–14) | [image]
Abbreviated name: | [^99m^Tc]Demobesin 1 | [image]
Synonym: | | [image]
Agent Category: | Peptide | [image]
Target: | Gastrin-releasing peptide receptor (GRPR) | [image]
Target Category: | Receptor | [image]
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging | [image]
Source of signal / contrast: | ^99m^Tc | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of [^99m^Tc]Demobesin 1. Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) for more information about gastrin-releasing peptide receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22bombesin%22%25GRPR%20imaging)]

[^99m^Tc-N_4_^0-1^-bzlg^0^,D-Phe^6^,Leu-NHEt^13^,des-Met^14^]Bombesin (6-14) ([^99m^Tc]Demobesin 1) is a bombesin (BN) derivative that was synthesized and labeled with ^99m^Tc by Nock et al. for molecular imaging of tumors expressing gastrin-releasing peptide receptor (GRPR) (1).

BN is an amphibian neuropeptide consisting of 14 amino acids (pGlu-Gln-Arg-Leu-Gly-Asn-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_) (2,3), which was first isolated from frog skin in 1970 (4). The search for its mammalian counterpart led to the discovery of gastrin-releasing peptide (GRP), which consists of 27 amino acids. GRP and BN share an identical C-terminal region (-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_) which is necessary for receptor binding and signal transduction (5,6). In addition to the release of gastrin, GRP and BN-like peptides also produce a wide range of other biological responses in diverse tissues, such as secretion of endocrine and exocrine glands, maintenance of circadian rhythm, regulation of satiety, and contraction of smooth muscles (7). They also act as potential growth factors for both normal and cancer cells (3, 5, 6). There are four members of the BN receptor family, including three mammalian receptors: GRPR (BB_2_ or BRS2; 384 amino acids), neuromedin B receptor (NMBR, BB_1_, or BRS1; 390 amino acids), and BN-like receptor 3 (BB_3_, BRS3, or orphan; 399 amino acids) (5, 7, 8); the fourth receptor (BB_4_) has only been found in amphibians. GRPR is the only well characterized receptor of this family. GRPR is a glycosylated, 7-transmembrane, G-protein–coupled receptor that, upon binding with its ligands, gives rise to a complex cascade of intracellular reactions. It is normally found in non-neuroendocrine tissues of the breast and pancreas and in neuroendocrine cells of the brain, gastrointestinal tract, lung, and prostate (9). Interestingly, GRPR is overexpressed in prostate cancer as well as in tumors of the breast, lung, pancreas, ovary, kidney, and gastrointestinal tract. It has been reported that GRPR is expressed at a high density in the intraepithelial neoplasia and primary carcinoma of the prostate, whereas normal prostate tissue and, in most cases, benign prostate hyperplasia are predominantly negative for GRPR (10-13).

GRPR has attracted significant interest as a target for tumor detection, tumor staging, and evaluation of tumor response to therapy (5, 6, 8, 11). A large number of BN derivatives have been developed, and they have been labeled with ^99m^Tc, ^177^Lu, ^67^Ga, and ^111^In for single-photon emission computed tomography and with ^64^Cu, ^68^Ga, and ^18^F for positron emission tomography. The published BN derivatives can be generally classified as truncated BN (6–14 or 7–14) or full-length BN (1-14) analogs (10, 12-18). The truncated BN analogs seem to be favorable for in vivo applications because they are usually more stable than the full-length tetradecapeptides and still bind to the GRPR adequately. However, the full-length peptides offer different labeling methods by attachment of functional groups to the amino acid 1 to 6. In many cases, the amino acids on positions 13 (Leu) and 14 (Met) have been replaced by unnatural amino acids (cyclohexylalanine (CyHAla) and norleucine (Nle)), and Lys has been placed on position 3 for attachment of radiolabels with reactive esters. Spacers, chelators, or radiometals have also been widely used for conjugation and for favorable kinetics (19). The BN derivatives can also be divided into agonists and antagonists (1, 20, 21). By far, most BN derivatives are agonists. Agonists are internalized into and accumulate within cells, and it has been assumed that they exhibit higher uptake by cancer cells than antagonists. However, some reports have shown that uptake of antagonists is much higher than that of agonists because antagonists may have stronger binding for the GRPR than agonists (1, 20).

An optimal BN-like radiotracer needs to meet several requirements: high affinity for GRPR, with rapid and specific tumor uptake; high hydrophilicity, with preferred renal excretion and low hepatobiliary excretion; and high stability but relatively rapid clearance from blood (6). Despite a large number of published derivatives, a valid comparison among them for the feasibility of tumor imaging is difficult because standardization between studies is lacking. Generally speaking, the majority of the radiotracers have relatively high renal and hepatic uptake, resulting in low tumor/liver and tumor/kidney ratios. Nock et al. developed a GRPR antagonist, [^99m^Tc]Demobesin 1, and further tested its biodistribution and feasibility of imaging GRPR-expressing tumors (1).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=demobesin)]

Demobesin 1 peptide was synthesized in two consecutive steps: coupling and deprotection (1). The tetraamine chelator precursor N,N’,N’’,N’’’-tetrakis-(tert-butoxycarbonyl)-6-{p-[(carboxymethoxy)acetyl]aminobenzyl}-1,4,8,11-tetraazaundecane (N_4_(Boc)_4_-bzlg) was first coupled to the N-terminal of the BN antagonist [D-Phe^6^,Leu-NHEt^13^,des-Met^14^]BN(6–14) through the coupling agent O-(7-azabenzotriazolyl-1,1,3,3-tetramethylammonium hexafluorophosphate. The Boc groups were then removed with trifluoroacetic acid treatment. The peptide conjugate, Demobesin 1, was purified with semipreparative reverse-phase high-performance liquid chromatography (RP-HPLC). The overall yield of Demobesin 1 was ~70%. For radiolabeling, the lyophilized peptide was dissolved in acetic acid/EtOH (8/2 v/v), followed by addition of sodium citrate, pertechnetate generator eluate, and freshly prepared ethanolic SnCl_2_ solution. The mixture was left to react for 30 min at ambient temperature and was then brought to pH 7 by addition of HCl before RP-HPLC purification of the [^99m^Tc]Demobesin 1. Radiochemical analysis showed that the specific activity and radiochemical yield of [^99m^Tc]Demobesin 1 were 37 GBq/μmol (1 Ci/μmol) and >96%, respectively. [^99m^Tc]Demobesin 1 was stable in the open reaction vial for at least 6 h after labeling. The [^99g^Tc]Demobesin 1 was prepared with similar protocol to that for its [^99m^Tc]Demobesin 1 counterpart at tracer level.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=demobesin)]

The metabolic stability of [^99m^Tc]Demobesin 1 was evaluated in mouse plasma and kidney homogenates (1). After incubation in mouse plasma at 37°C, >85% of the [^99m^Tc]Demobesin 1 remained intact after 1 h. During the first 15 min of incubation, the intact peptide fraction exceeded 90%. Rapid degradation was observed in the kidney preparation, with <5% intact peptide detected after just 5 min of incubation. This result was consistent with the analysis of urine collected 30 min after injection of [^99m^Tc]Demobesin 1 in mice, which showed complete degradation of the original peptide. Two major hydrophilic metabolites were detected in the urine; these were, however, unrelated to ^99m^TcO_4_^-^.

The binding capability and internalization of [^99m^Tc]Demobesin 1 for GRPR were investigated with PC-3 cell membrane homogenates, human tumor biopsy specimens, and PC-3 culture cells (1). [Tyr^4^]BN peptide served as the positive control and [^125^I-Tyr^4^]BN served as the specific radioligand, where [Tyr^4^]BN was Pyr-Gln-Arg-Tyr-Gly-Asn-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. Competitive binding assays in PC-3 membrane preparations demonstrated that [^125^I-Tyr^4^]BN was displaced by Demobesin 1 from BN binding sites in a monophasic and dose-dependent manner. The 50% inhibitory concentration (IC_50_) value was 0.7 ± 0.08 nmol, comparable to the IC_50_ value of [Tyr^4^]BN (1.5 ± 0.20 nmol). The equilibrium dissociation constant and maximal binding value of [^99m^Tc/^99g^Tc]Demobesin 1 were 0.67 ± 0.10 nmol and 262 ± 13 fmol/mg, respectively. Competition binding experiments in human tumor biopsy specimens showed that Demobesin 1 had high binding affinity in the GRPR-expressing prostate cancer, but not in the NMBR-expressing (gut carcinoid) and BB_3_-expressing (lung carcinoid) tumors. The IC_50_ values were 2.6 ± 0.2 nmol in prostate cancer (n = 5) and >1,000 nmol in BB_3_- or NMBR-expressing tumors (n = 3). Internalization was rapid, but only a small portion (~25% radioactivity) of the [^99m^Tc]Demobesin 1 was detected within the cells after 120 min of incubation with PC-3 culture cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=demobesin)]

Nock et al. investigated the biodistribution of [^99m^Tc]Demobesin 1 in healthy, male, Swiss albino mice (n = 30) and in female, Swiss, nu/nu mice bearing subcutaneous human PC-3 xenografts (n = 4–6/time point) (1). Each animal was given 148–185 kBq (4–5 μCi) [^99m^Tc]Demobesin 1 (10 pmol of total peptide) via the tail vein. In healthy mice, rapid clearance of the [^99m^Tc]Demobesin 1 was observed via the kidneys, with a small portion of liver uptake. High accumulation in the GRPR-expressing pancreas was detected up to 58.7 ± 6.1% injected dose per gram of tissue (ID/g) at 30 min after injection. The intestine, another GRPR-expressing organ, also had a relatively high accumulation level (7.53 ± 0.85% ID/g at 30 min after injection). Pretreatment of the mice with intraperitoneal administration of 1 mg [Tyr^4^]BN 35 min before injection strongly blocked uptake of [^99m^Tc]Demobesin 1 in both organs, showing uptake levels of only 2.7 ± 1.1% ID/g in the pancreas and 2.26 ± 0.56% ID/g in the intestine at 30 min after injection (n = 4–6 animals). In mice with PC-3 xenografts (n = 4–6/time point), the uptake of [^99m^Tc]Demobesin 1 was already evident at 1 h after injection in both pancreas (79.5 ± 0.8% ID/g) and tumor (16.2 ± 3.1% ID/g). The high tumor uptake remained at this level (15.61 ± 1.19% ID/g) up to 4 h after injection. Rapid clearance of the [^99m^Tc]Demobesin 1, predominantly via the kidneys, resulted in increased high tumor/background ratios over time. The tumor/nontarget tissue ratios were 12.9 ± 3.3 for the blood, 67.6 ± 13.7 for the muscle, 2.0 ± 0.5 for the liver, and 2.0 ± 0.5 for the kidneys at 1 h after injection, and 23.1 ± 3.6 for the blood, 206.0 ± 21.1 for the muscle, 2.2 ± 0.3 for the liver, and 2.7 ± 0.4 for the kidneys at 4 h after injection.

Blocking studies were performed with intravenous administration of 250 μg [Tyr^4^]BN along with [^99m^Tc]Demobesin 1 or intraperitoneal administration of 1 mg [Tyr^4^]BN 35 min before the administration of [^99m^Tc]Demobesin 1 (n = 4–6 mice/group) (1). The uptake of [^99m^Tc]Demobesin 1 in both pancreas and tumor was blocked by the [Tyr^4^]BN. The uptake level was only 3.26 ± 0.71% ID/g in the pancreas and 2.34 ± 0.33% ID/g in the tumor at 1 h after injection. The tumor/blocked tumor ratios were 6.9 ± 1.3 and 7.7 ± 1.2% ID/g at 1 h and 4 h, respectively.

Static imaging studies were performed in two mice bearing PC-3 tumors with administration of the [^99m^Tc]Demobesin 1 alone in one mouse (unblocked mouse) and together with 250 μg [Tyr^4^]BN in another mouse (blocked mouse) (1). The images obtained at 1.5 h after injection clearly delineated the tumor in the unblocked mouse. In contrast, the tumor was not visualized in the blocked mouse.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Nock B., Nikolopoulou A., Chiotellis E., Loudos G., Maintas D., Reubi J.C., Maina T. (2003). [99mTc]Demobesin 1, a novel potent bombesin analogue for GRP receptor-targeted tumour imaging. Eur J Nucl Med Mol Imaging.
2 Maina T., Nock B.A., Zhang H., Nikolopoulou A., Waser B., Reubi J.C., Maecke H.R. (2005). Species differences of bombesin analog interactions with GRP-R define the choice of animal models in the development of GRP-R-targeting drugs. J Nucl Med.
3 Smith C.J., Volkert W.A., Hoffman T.J. (2003). Gastrin releasing peptide (GRP) receptor targeted radiopharmaceuticals: a concise update. Nucl Med Biol.
4 Erspamer V., Erpamer G.F., Inselvini M. (1970). Some pharmacological actions of alytesin and bombesin. J Pharm Pharmacol.
5 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
6 Ananias H.J., de Jong I.J., Dierckx R.A., van de Wiele C., Helfrich W., Elsinga P.H. (2008). Nuclear imaging of prostate cancer with gastrin-releasing-peptide-receptor targeted radiopharmaceuticals. Curr Pharm Des.
7 Ischia J., Patel O., Shulkes A., Baldwin G.S. (2009). Gastrin-releasing peptide: different forms, different functions. Biofactors.
8 Maina T., Nock B., Mather S. (2006). Targeting prostate cancer with radiolabelled bombesins. Cancer Imaging.
9 Weber H.C. (2009). Regulation and signaling of human bombesin receptors and their biological effects. Curr Opin Endocrinol Diabetes Obes.
10 Yang Y.S., Zhang X., Xiong Z., Chen X. (2006). Comparative in vitro and in vivo evaluation of two 64Cu-labeled bombesin analogs in a mouse model of human prostate adenocarcinoma. Nucl Med Biol.
11 Liu S., Edwards D.S., Barrett J.A. (1997). 99mTc labeling of highly potent small peptides. Bioconjug Chem.
12 Zhang X., Cai W., Cao F., Schreibmann E., Wu Y., Wu J.C., Xing L., Chen X. (2006). 18F-labeled bombesin analogs for targeting GRP receptor-expressing prostate cancer. J Nucl Med.
13 Schroeder R.P., van Weerden W.M., Bangma C., Krenning E.P., de Jong M. (2009). Peptide receptor imaging of prostate cancer with radiolabelled bombesin analogues. Methods.
14 Chen X., Park R., Hou Y., Tohme M., Shahinian A.H., Bading J.R., Conti P.S. (2004). microPET and autoradiographic imaging of GRP receptor expression with 64Cu-DOTA-[Lys3]bombesin in human prostate adenocarcinoma xenografts. J Nucl Med.
15 Hohne A., Mu L., Honer M., Schubiger P.A., Ametamey S.M., Graham K., Stellfeld T., Borkowski S., Berndorff D., Klar U., Voigtmann U., Cyr J.E., Friebe M., Dinkelborg L., Srinivasan A. (2008). Synthesis, 18F-labeling, and in vitro and in vivo studies of bombesin peptides modified with silicon-based building blocks. Bioconjug Chem.
16 Li Z.B., Wu Z., Chen K., Ryu E.K., Chen X. (2008). 18F-labeled BBN-RGD heterodimer for prostate cancer imaging. J Nucl Med.
17 Prasanphanich A.F., Retzloff L., Lane S.R., Nanda P.K., Sieckman G.L., Rold T.L., Ma L., Figueroa S.D., Sublett S.V., Hoffman T.J., Smith C.J. (2009). In vitro and in vivo analysis of [(64)Cu-NO2A-8-Aoc-BBN(7-14)NH(2)]: a site-directed radiopharmaceutical for positron-emission tomography imaging of T-47D human breast cancer tumors. Nucl Med Biol.
18 Santos-Cuevas C.L., Ferro-Flores G., Arteaga de Murphy C., Ramirez Fde M., Luna-Gutierrez M.A., Pedraza-Lopez M., Garcia-Becerra R., Ordaz-Rosado D. (2009). Design, preparation, in vitro and in vivo evaluation of (99m)Tc-N2S2-Tat(49-57)-bombesin: a target-specific hybrid radiopharmaceutical. Int J Pharm.
19 Fragogeorgi, E.A., C. Zikos, E. Gourni, P. Bouziotis, M. Paravatou-Petsotas, G. Loudos, N. Mitsokapas, S. Xanthopoulos, M. Mavri-Vavayanni, E. Livaniou, A.D. Varvarigou, and S.C. Archimandritis, Spacer Site Modifications for the Improvement of the in Vitro and in Vivo Binding Properties of (99m)Tc-N(3)S-X-Bombesin[2-14] Derivatives. Bioconjug Chem, 2009
20 Cescato R., Maina T., Nock B., Nikolopoulou A., Charalambidis D., Piccand V., Reubi J.C. (2008). Bombesin receptor antagonists may be preferable to agonists for tumor targeting. J Nucl Med.
21 Nock B.A., Nikolopoulou A., Galanis A., Cordopatis P., Waser B., Reubi J.C., Maina T. (2005). Potent bombesin-like peptides for GRP-receptor targeting of tumors with 99mTc: a preclinical study. J Med Chem.